# N-(Morpholin-4-yl)-5-(4-[^123^I]iodophenyl)-1-(2,4-dichlorophenyl)-4-methyl-1H-pyrazole-3-carboxamide

Chemical name: | N-(Morpholin-4-yl)-5-(4-[^123^I]iodophenyl)-1-(2,4-dichlorophenyl)-4-methyl-1H-pyrazole-3-carboxamide
Abbreviated name: | [^123^I]AM281
Synonym:
Agent Category: | Compound
Target: | Cannabinoid CB1receptors
Target Category: | Receptor binding
Method of detection: | SPECT, gamma planar
Source of signal: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AM281%20and%20%28123I%20or%20124I%29)]

There are two subtypes of cannabinoid receptors in mammalian tissues: CB1 and CB2 (1, 2). CB1 receptors are expressed abundantly in neuronal terminals in the central nervous system (CNS) and peripheral tissues to inhibit neurotransmitter release. CB1 receptors are found predominately in the striatum, hippocampus, substantia nigra, globus pallidus, and cerebellum. CB2 receptors are present mainly on immune cells to modulate cytokine release. Both receptor subtypes are coupled through G_i/o_ proteins to inhibit adenylate cyclase and to modulate potassium and calcium channels. CB1 receptors have been demonstrated to be involved in analgesia, regulation of food intake, and control of movement in normal subjects (3). Alteration of CB1 receptor function has been implicated in a number of human diseases such as depression, schizophrenia, and obesity (4-6).

Δ9-Tetrahydrocannabinol (THC) is a major active cannabinoid that is found in marijuana and activates CB1 receptors (7). THC has a very high lipophilicity (log P, 7), which causes imaging studies that use radiolabeled THC to be unsuccessful because of high nonspecific binding in the brain and slow brain entry. However, high lipophilicity is essential for binding to CB1 receptors, and moderate lipophilicity is required for crossing the blood–brain barrier (BBB). Existing radiolabeled ligands are mainly analogs of the antagonist rimonabant (SR141716A) and the agonist WIN 55,212-2; however, these ligands also exhibit high nonspecific binding, which limits their application in imaging (8). Therefore, there is a need to lower the lipophilicity of the radioligands with little effect on binding affinity and ability to cross the BBB. N-(Morpholin-4-yl)-5-(4-iodophenyl)-1-(2,4-dichlorophenyl)-4-methyl-1H-pyrazole-3-carboxamide (AM281) is a potent and selective CB1 antagonist with nanomolar affinity and lower lipophilicity than its analog, SR141716A. N-(Morpholin-4-yl)-5-(4-[^123^I]iodophenyl)-1-(2,4-dichlorophenyl)-4-methyl-1H-pyrazole-3-carboxamide ([^123^I]AM281) is being developed as a single photon emission computed tomography (SPECT) agent for the non-invasive study of CB1 receptors in the brain (9, 10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AM281%20and%20%28123I%20or%20124I%29%20and%20synthesis)]

Lan et al. (10) reported synthesis of [^123^I]AM281 by radioiododestannylation reaction of the tributyltin precursor with [^123^I]iodide in the presence of phosphoric acid and chloramine-T. Radiochemical yields were 50–60% after high-performance liquid chromatography purification. Specific activities were >185 GBq/μmol (>5 Ci/μmol) with a radiochemical purity of >95%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AM281%20and%20%28123I%20or%20124I%29%20and%20in%20vitro)]

Lan et al. (10) reported that AM281 had an inhibitory constant (K_i_) value of 12 nM for CB1 receptors in rat forebrain membranes and a K_i_ value of 4,200 nM for CB2 receptors in mouse spleen membranes, with a ratio of CB2/CB1 K_i_ values of 340. THC had a K_i_ value of 41 nM for CB1 receptors. The lipophilicity values were 3.7 for AM281 and 4.8 for SR141716A. Gatley et al. (9) reported that AM281 was 8-fold less potent than SR141716A in displacing [^3^H]SR141716A from binding CB1 receptors in mouse cerebellum membranes. CB1 binding of [^123^I]AM281 was inhibited by SR141716A, WIN 55,212-2, and THC with K_i_ values of 1.8, 84, and 208, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AM281%20and%20%28123I%20or%20124I%29%20and%20rodentia)]

Gatley et al. (9) showed that there was good uptake of radioactivity in the mouse cerebellum after injection of [^123^I]AM281, which reached a peak value of ~3.3% injected dose/g (ID/g) at 30 min and declining to ~1.9% ID/g at 60 min. The brain stem reached a peak value of ~2.6% ID/g at 30 min and declined more rapidly than the cerebellum to <1% ID/g at 60 min. Pretreatment with 2 mg/kg SR141716A before [^123^I]AM281 injection reduced the cerebellum and brain stem uptakes to similar levels. Ex vivo autoradiography of rat brain showed the highest radioactivity in the substantia nigra, globus pallidus, and cerebellum, followed by cortex, striatum, thalamus, and brain stem at 120 min after [^123^I]AM281 injection, consistent with the CB1 distribution in the brain.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AM281%20and%20%28123I%20or%20124I%29%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AM281%20and%20%28123I%20or%20124I%29%20and%20monkey)]

Biodistribution PET studies in anesthetized baboons injected with [^123^I]AM281 were performed by Gatley et al. (9). These studies demonstrated the highest uptake in the cerebellum, followed by the cortex and striatum. The peak level of radioactivity was reached in the cerebellum at ~20 min and declined with a half-life of 90 min. Pretreatment with SR141716A 10 min before [^123^I]AM281 or 30 min after [^123^I]AM281 accelerated the decline from the cerebellum between 20 and 60 min after injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AM281%20and%20%28123I%20or%20124I%29%20and%20human)]

Berding et al. (11) evaluated specific binding of [^123^I]AM281 to CB1 receptors by SPECT imaging in six Tourette syndrome patients before and after THC treatment. The brain exhibited a low maximal uptake of 1.9% ID/g. Distribution volumes (DV) were obtained for the lentiform nuclei (3.5–3.8), occipital cortex (2.8–2.9), and white matter (3.0–3.1) using plasma input with the one-tissue compartment model and with Logan's graphical analysis. There were significantly lower DV values after therapy. However, using the occipital cortex or white matter as the reference region, no significant differences before or after therapy were detected in the lentiform nuclei by the specific to nonspecific partition coefficient V_3_” (0.19–0.31). Only one patient with a marked clinical response showed a clear decline in V_3_” value. After injection of [^123^I]AM281, 70–75% of the total radioactivity in the blood was intact parent compound at 10 min, and 55–60% at 3 h. The main radioactive metabolite was more hydrophilic than [^123^I]AM281. The organs that received the highest absorbed doses were found to be the upper large intestine (0.0461 mSv/MBq [170 mrem/mCi]), spleen (0.041 mSv/MBq [152 mrem/mCi]), and bone marrow (0.027 mSv/MBq [100 mrem/mCi]). The brain exhibited 0.0074 mSv/MBq (27 mrem/mCi). The effective dose was calculated as 0.011 mSv/MBq (40.7 mrem/mCi).

## NIH Support

DA-3801, DA-152, DA-6278, DA-7215, DA-7515, DA-9158

## References

1 Howlett A.C. Barth F. Bonner T.I. Cabral G. Casellas P. Devane W.A. Felder C.C. Herkenham M. Mackie K. Martin B.R. Mechoulam R. Pertwee R.G. International Union of Pharmacology.XXVII. Classification of cannabinoid receptors Pharmacol Rev 2002 54 2 161 202 12037135
2 Pertwee R.G. (1997). Pharmacology of cannabinoid CB1 and CB2 receptors. Pharmacol Ther.
3 Pertwee R.G. (2005). Pharmacological actions of cannabinoids. Handb Exp Pharmacol, (168): p. 1-51.
4 Gambi F., De Berardis D., Sepede G., Quartesan R., Calcagni E., Salerno R.M., Conti C.M., Ferro F.M. (2005). Cannabinoid receptors and their relationships with neuropsychiatric disorders. Int J Immunopathol Pharmacol.
5 De Vries T.J., Schoffelmeer A.N. (2005). Cannabinoid CB1 receptors control conditioned drug seeking. Trends Pharmacol Sci.
6 Guzman M., Sanchez C. (1999). Effects of cannabinoids on energy metabolism. Life Sci.
7 Martin B.R. (1986). Cellular effects of cannabinoids. Pharmacol Rev.
8 Gifford A.N., Makriyannis A., Volkow N.D., Gatley S.J. (2002). In vivo imaging of the brain cannabinoid receptor. Chem Phys Lipids.
9 Gatley S.J., Lan R., Volkow N.D., Pappas N., King P., Wong C.T., Gifford A.N., Pyatt B., Dewey S.L., Makriyannis A. (1998). Imaging the brain marijuana receptor: development of a radioligand that binds to cannabinoid CB1 receptors in vivo. J Neurochem.
10 Lan R., Gatley J., Lu Q., Fan P., Fernando S.R., Volkow N.D., Pertwee R., Makriyannis A. (1999). Design and synthesis of the CB1 selective cannabinoid antagonist AM281: a potential human SPECT ligand. AAPS PharmSci.
11 Berding G., Muller-Vahl K., Schneider U., Gielow P., Fitschen J., Stuhrmann M., Harke H., Buchert R., Donnerstag F., Hofmann M., Knoop B.O., Brooks D.J., Emrich H.M., Knapp W.H. (2004). [(123)I]AM281 single-photon emission computed tomography imaging of central cannabinoid CB(1) receptors before and after Delta(9)-tetrahydrocannabinol therapy and whole-body scanning for assessment of radiation dose in tourette patients. Biol Psychiatry.